# 1-(2,3-Dihydrobenzo[b][1,4]dioxin-6-yl)-4-((6-[^18^F]fluoropyridin-3-yl)methyl)piperazine

Chemical name: | 1-(2,3-Dihydrobenzo[b][1,4]dioxin-6-yl)-4-((6-[^18^F]fluoropyridin-3-yl)methyl)piperazine
Abbreviated name: | [^18^F]3d
Synonym:
Agent category: | Compound
Target: | Dopamine D_4_ receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_-_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes have been classified into two subfamilies of D_1_-like (D_1_, D_5_) and D_2_-like (D_2_, D_3_, D_4_) dopamine receptors. D_1_-Like and D_2_-like receptors exert synergistic as well as opposite effects at the biochemical and overall system levels. A great majority of striatal D_1_ and D_2/3_ receptors are localized postsynaptically on the caudate-putamen neurons, and to a lesser extent presynaptically on nigrostriatal axons. On the other hand, D_4_ receptors are mostly found in the extrastriatal regions of the brain, such as the cortex, hippocampus, thalamus, and medulla. These areas are believed to control emotion and cognition.

In addition to D_2_ receptors, D_4_ receptors may play an important role in the pathophysiology of schizophrenia, as suggested by clinical studies of the atypical neuroleptic clozapine in patients (5, 6). Clozapine is not only effective against positive symptoms of schizophrenia, but it is also efficacious against the negative symptoms. Clozapine has a 10-fold greater affinity for D_4_ receptors than for D_2_ receptors (7). However, it also has high affinities for 5-HT_1A,1B,2A,2C,6,7_, α_1A,2A,2C_, muscarinic M_1_, and histamine H_1_ receptors. The neurophysiological role of D_4_ receptors remains to be defined. Thus, there is a need to for selective ligands to investigate the pharmacological role of D_4_ receptors. There have been several attempts to develop specific D_4_ radioligands for use with positron emission tomography (PET) imaging of D_4_ receptors (8-10). However, none has proved suitable because of a lack of selectivity and other pharmacological issues. Kugler et al. (11) reported that 1-(2,3-dihydrobenzo[b][1,4]dioxin-6-yl)-4-((6-fluoropyridin-3-yl)methyl)piperazine (3d) is a potent antagonist of D_4_ receptors, with >1,100-fold selectivity over D_2_ and D_3_ receptors. This led to the development of 1-(2,3-dihydrobenzo[b][1,4]dioxin-6-yl)-4-((6-[^18^F]fluoropyridin-3-yl)methyl)piperazine ([^18^F]3d) as a potential D_4_ receptor radioligand for use with PET imaging of D_4_ receptors in the brain.

### Related Resource Links:

- Chapters in MICAD (dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814), D_4_ receptor (http://www.ncbi.nlm.nih.gov/gene/1815))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451), D_4_ receptor (http://www.ncbi.nlm.nih.gov/omim/126452))
- Clinical trials (dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20synthesis%5bAll%20Fields%5d)]

6-[^18^F]Fluoronicotinaldehyde was produced via nucleophilic aromatic substitution of the chloro derivative with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide (11). [^18^F]3d radiosynthesis was accomplished by the reductive amination of 6-[^18^F]fluoronicotinaldehyde with 1-(1,4-benzodioxine-6-yl)piperazine in one-pot synthesis, followed by high-performance liquid chromatography purification. The overall radiochemical yield of [^18^F]3d was 15 ± 5%, with a specific radioactivity of 60 GBq/µmol (1.6 Ci/µmol) at the end of synthesis. The radiochemical purity was >98%, with a total synthesis time of ~80 min. Compound 3d exhibited a logD_7.4_ value of 1.81 ± 0.05.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20in%20vitro)]

Compound 3d was reported to have high binding affinities to D_4_ receptor sites but not to D_1/2/3_ receptors in recombinant cell lines (11). The K_i_ values for D_1_, D_2long_, D_2short_, D_3_, and D_4_ receptors were 35,000, 29,000, 45,000, 17,000, and 1.5 ± 0.7 nM, respectively. The D_2_/D_4_K_i_ ratio was calculated to be >2,000. Compound 3d exhibited little affinity for 5-HT_1A_, 5-HT_2_, and sigma-1 receptors (K_i_ values > 5,800 nM). In vitro autoradiography studies of rat brain sections showed that [^18^F]3d (5 nM) displayed radioactivity throughout the brain with a distinct high accumulation of radioactivity in the colliculus and cerebellum. Compound 3d (10 µM) blocked the radioactivity to homogeneity. Non-specific binding of [^18^F]3d on horizontal rat brain slices was ~7%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20rodentia)]

Kugler et al. (11) performed ex vivo biodistribution studies in normal mice (n = 3/group) at 5, 10, 15, and 30 min after intravenous injection of 1.1–2.6 MBq (0.03–0.07 mCi) [^18^F]3d. Radioactivity accumulation in the brain was 4.93%, 2.85%, 2.27%, and 1.47% injected dose per gram (ID/g) at 5, 10, 15, and 30 min, respectively. The organ with the highest radioactivity accumulation at 30 min was the liver (7.79% ID/g), followed by the pancreas (7.43% ID/g), kidney (6.03% ID/g), intestine (4.47% ID/g), spleen (3.13% ID/g), lung (2.68% ID/g), heart (1.13% ID/g), bone (0.93% ID/g), and blood (0.53% ID/g). [^18^F]3d remained >98% and ~50% intact in the brain and plasma, respectively, at 10 min after injection. Ex vivo autoradiography studies of the brain at 15 min showed high radioactivity in the colliculus, cerebral cortex, and cerebellum, with moderate radioactivity in the hippocampus and striatum. No blocking studies were performed. Further studies are needed to define the selectivity of [^18^F]3d as a D_4_ PET radioligand in vivo.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20(dog%20or%20pig%20or%20rabbit%20ot%20sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Dopamine%20D4%20fluorine%20radioisotopes%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 Seeman P., Guan H.C., Van Tol H.H. (1993). Dopamine D4 receptors elevated in schizophrenia. Nature.
6 Seeman P., Guan H.C., Van Tol H.H., Niznik H.B. (1993). Low density of dopamine D4 receptors in Parkinson's, schizophrenia, and control brain striata. Synapse.
7 Van Tol H.H., Bunzow J.R., Guan H.C., Sunahara R.K., Seeman P., Niznik H.B., Civelli O. (1991). Cloning of the gene for a human dopamine D4 receptor with high affinity for the antipsychotic clozapine. Nature.
8 Bender D., Holschbach M., Stocklin G. (1994). Synthesis of n.c.a. carbon-11 labelled clozapine and its major metabolite clozapine-N-oxide and comparison of their biodistribution in mice. Nucl Med Biol.
9 Boy C., Klimke A., Holschbach M., Herzog H., Muhlensiepen H., Rota Kops E., Sonnenberg F., Gaebel W., Stocklin G., Markstein R., Muller-Gartner H.W. (1998). Imaging dopamine D4 receptors in the living primate brain: a positron emission tomography study using the novel D1/D4 antagonist [11C]SDZ GLC 756. Synapse.
10 Zhang M.R., Haradahira T., Maeda J., Okauchi T., Kawabe K., Noguchi J., Kida T., Suzuki K., Suhara T. (2002). Syntheses and pharmacological evaluation of two potent antagonists for dopamine D4 receptors: [11C]YM-50001 and N-[2-[4-(4-Chlorophenyl)-piperizin-1-yl]ethyl]-3-[11C]methoxybenzamide. Nucl Med Biol.
11 Kugler F., Sihver W., Ermert J., Hubner H., Gmeiner P., Prante O., Coenen H.H. (2011). Evaluation of 18F-labeled benzodioxine piperazine-based dopamine D4 receptor ligands: lipophilicity as a determinate of nonspecific binding. J Med Chem.